# 4-(3-((5-(2-[^18^F]Fluoroethoxy)pyridine-2-yl)oxy)benzylidene)-N-(pyridazin-3-yl)piperidine-1-carboxamide

Chemical name: | 4-(3-((5-(2-[^18^F]Fluoroethoxy)pyridine-2-yl)oxy)benzylidene)-N-(pyridazin-3-yl)piperidine-1-carboxamide
Abbreviated name: | [^18^F]PF-9811
Synonym:
Agent category: | Compound
Target: | Fatty acid amide hydrolase (FAAH)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PF-9811)]

Fatty acid amide hydrolase (FAAH) is an integral membrane-bound serine hydrolase and a part of the endocannabinoid system (ECS), which comprises the cannabinoid receptors (CB1 and CB2), endogenous ligands termed endocannabinoids (anandamide and oleamide), transporters, and enzymes (1, 2). FAAH plays a key role in the hydrolysis of a number of primary and secondary fatty acid amides, controlling the levels of the neuromodulatory endocannabinoids in the ECS (3, 4). FAAH is widely expressed in many tissues, with the highest levels in the liver and brain (5). Genetic or pharmacological inactivation of FAAH in the brain leads to analgesic, anti-inflammatory, anxiolytic, and anti-depression effects in animal models (6-8).

Cyclohexylcarbamic acid 3'-carbamoylbiphenyl-3-yl ester (URB597) is an irreversible, substrate-like inhibitor of FAAH involving carbamylation of the catalytic nucleophilic Ser^241^ and the O-biaryl group as the leaving group (9-11). On the basis of the structure of URB597, Wyffels et al. (11) prepared biphenyl-3-yl-4-[^11^C]methoxyphenylcarbamate ([^11^C]-1) for in vivo positron emission tomography (PET) imaging studies of the brain FAAH in mice. It was proposed that the carbamylation of Ser^241^ would leave the [^11^C]-methoxyanilino group bound to the FAAH for visualization of FAAH in the brain. However, the results of in vitro and ex vivo studies indicated that [^11^C]-1 is a reversible inhibitor of FAAH, and the rapid brain washout of the tracer limits its utility as a PET agent for in vivo measurements of FAAH. Wilson et al. (10) reported the ^11^C-radiolabeling of a close analog of URB597, 6-hydroxy-[1,1'-biphenyl]-3-yl-cyclohexylcarbamate (URB694), yielding [^11^C-carbonyl]URB694 ([^11^C]CURB) for PET imaging of FAAH in the brain. [^11^C]CURB showed good brain accumulation with regional heterogeneity, irreversibility, and specific binding to FAAH in vivo in rats.

Skaddan et al. (9) prepared 4-(3-((5-(2-[^18^F]fluoroethoxy)pyridine-2-yl)oxy)benzylidene)-N-(pyridazin-3-yl)piperidine-1-carboxamide ([^18^F]PF-9811) for use with in vivo PET imaging of FAAH. PF-9811 is a close analog of 4-(3-((5-(2-trifluoromethyl)pyridine-2-yl)oxy)benzylidene)-N-(pyridazin-3-yl)piperidine-1-carboxamide (PF-04457845), which is a clinical candidate for treatment of inflammatory and non-inflammatory pain. [^18^F]PF-9811 showed good brain accumulation, with regional heterogeneity and specific binding to FAAH in vivo in rats.

### Related Resource Links:

- Chapters in MICAD (FAAH (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=FAAH+AND+micad%5Bbook%5D))
- Gene information in NCBI (FAAH (http://www.ncbi.nlm.nih.gov/gene/2166))
- Articles in Online Mendelian Inheritance in Man (OMIM) (FAAH (http://omim.org/entry/602935))
- Clinical trials (FAAH (http://www.clinicaltrials.gov/ct2/results?term=FAAH&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PF-9811%20and%20synthesis)]

Skaddan et al. (9) synthesized [^18^F]PF-9811 via a 3-step, one-pot reaction sequence in 87 min from the end of bombardment. [^18^F]PF-9811 was purified with high-performance liquid chromatography with >98% radiochemical purity. The specific activity of [^18^F]PF-9811 was >444 GBq/μmol (12 Ci/µmol) at the end of synthesis. The LogP_7.4_ value of [^18^F]PF-9811 was 3.14 ± 0.02.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PF-9811%20and%20in%20vitro)]

Skaddan et al. (9) showed that unlabeled PF-04457845 and PF-9811 inhibited FAAH activity in mouse brain homogenates with IC_50_ values of 3.2 and 16 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PF-9811%20and%20rodentia)]

Ex vivo biodistribution studies in normal male rats (n = 4/group) were performed at 10, 60, and 90 min after intravenous injection of ~70 MBq (2.1 mCi) [^18^F]PF-9811 (0.4 nmol/kg) (9). The accumulation level of radioactivity was the highest in the cortex and cerebellum, followed by the hippocampus, striatum, hypothalamus, thalamus, and brain stem, with standard uptake values (SUVs) of 0.32–0.67 at 10 min, and the accumulation gradually increased to 0.39–0.86 SUV at 90 min. The distribution of radioactivity in the brain regions is in agreement with the known distribution of FAAH in the rat brain. The SUVs in the liver and bone at 90 min were 16.1 and 0.16 (indicating minimal defluorination), respectively. Radioactivity in the blood was lower than in the brain. The brain/blood ratios increased from 2.7 at 10 min to 12.9 at 90 min after injection. Pretreatment (60 min) with PF-04457845 (1 mg/kg, oral) inhibited the radioactivity levels by 37%–73%, depending on the brain regions, and 74% in the liver at 90 min. The specific/non-specific ratios were 2.3, 2.4, and 2.6 for the hippocampus, cerebellum, and cortex, respectively.

PET imaging studies were performed in six male rats cannulated in the jugular vein; scans were performed at 1, 2, 5, 10, 15, 20, 30, 45, 60, and 90 min after injection of ~74 MBq (2 mCi) [^18^F]PF-9811 (9). The highest radioactivity levels were observed in the cortex, cerebellum, and hippocampus. Radioactivity accumulation reached a plateau by ~60 min and gradually increased up to 90 min. Pretreatment (60 min) with PF-04457845 (1 mg/kg, oral) inhibited the radioactivity levels in the cortex, cerebellum, and hippocampus by ~40%–50% at 90 min based on image quantitation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PF-9811%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PF-9811%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PF-9811%20and%20human)]

No publication is currently available.

## References

1 Bambico F.R., Duranti A., Tontini A., Tarzia G., Gobbi G. (2009). Endocannabinoids in the treatment of mood disorders: evidence from animal models. Curr Pharm Des.
2 Thomas E.A., Cravatt B.F., Danielson P.E., Gilula N.B., Sutcliffe J.G. (1997). Fatty acid amide hydrolase, the degradative enzyme for anandamide and oleamide, has selective distribution in neurons within the rat central nervous system. J Neurosci Res.
3 Fowler C.J., Naidu P.S., Lichtman A., Onnis V. (2009). The case for the development of novel analgesic agents targeting both fatty acid amide hydrolase and either cyclooxygenase or TRPV1. Br J Pharmacol.
4 Naidu P.S., Kinsey S.G., Guo T.L., Cravatt B.F., Lichtman A.H. (2010). Regulation of inflammatory pain by inhibition of fatty acid amide hydrolase. J Pharmacol Exp Ther.
5 Alexander J.P., Cravatt B.F. (2005). Mechanism of carbamate inactivation of FAAH: implications for the design of covalent inhibitors and in vivo functional probes for enzymes. Chem Biol.
6 Ahn K., Smith S.E., Liimatta M.B., Beidler D., Sadagopan N., Dudley D.T., Young T., Wren P., Zhang Y., Swaney S., Van Becelaere K., Blankman J.L., Nomura D.K., Bhattachar S.N., Stiff C., Nomanbhoy T.K., Weerapana E., Johnson D.S., Cravatt B.F. (2011). Mechanistic and pharmacological characterization of PF-04457845: a highly potent and selective fatty acid amide hydrolase inhibitor that reduces inflammatory and noninflammatory pain. J Pharmacol Exp Ther.
7 Basso E., Duranti A., Mor M., Piomelli D., Tontini A., Tarzia G., Traldi P. (2004). Tandem mass spectrometric data-FAAH inhibitory activity relationships of some carbamic acid O-aryl esters. J Mass Spectrom.
8 Mor M., Rivara S., Lodola A., Plazzi P.V., Tarzia G., Duranti A., Tontini A., Piersanti G., Kathuria S., Piomelli D. (2004). Cyclohexylcarbamic acid 3'- or 4'-substituted biphenyl-3-yl esters as fatty acid amide hydrolase inhibitors: synthesis, quantitative structure-activity relationships, and molecular modeling studies. J Med Chem.
9 Skaddan M.B., Zhang L., Johnson D.S., Zhu A., Zasadny K.R., Coelho R.V., Kuszpit K., Currier G., Fan K.H., Beck E.M., Chen L., Drozda S.E., Balan G., Niphakis M., Cravatt B.F., Ahn K., Bocan T., Villalobos A. (2012). The synthesis and in vivo evaluation of [(18)F]PF-9811: a novel PET ligand for imaging brain fatty acid amide hydrolase (FAAH). Nucl Med Biol.
10 Wilson A.A., Garcia A., Parkes J., Houle S., Tong J., Vasdev N. (2011). [11C]CURB: Evaluation of a novel radiotracer for imaging fatty acid amide hydrolase by positron emission tomography. Nucl Med Biol.
11 Wyffels L., Muccioli G.G., Kapanda C.N., Labar G., De Bruyne S., De Vos F., Lambert D.M. (2010). PET imaging of fatty acid amide hydrolase in the brain: synthesis and biological evaluation of an 11C-labelled URB597 analogue. Nucl Med Biol.